# 1-[4-(3-[^18^F]Fluoropropoxy)-3-methoxyphenyl]-5-hydroxy-7-(4-hydroxy-3-methoxyphenyl)-1,4,6-heptatrien-3-one

Chemical name: | 1-[4-(3-[^18^F]fluoropropoxy)-3-methoxyphenyl]-5-hydroxy-7-(4-hydroxy-3-methoxyphenyl)-1,4,6-heptatrien-3-one
Abbreviated name: | [^18^F]Fluoropropyl-substituted curcumin
Synonym:
Agent Category: | Compound
Target: | Aggregates of ß-amyloid (Aß) peptides
Target Category: | Acceptor binding
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29Fluoropropyl-substituted%20curcumin)]

Alzheimer’s disease (AD) is a major neurodegenerative disease associated with an irreversible decline of mental functions and with cognitive impairment (1, 2). It is characterized by the presence, in the brain, of senile plaques of β-amyloid (Aβ) peptides with intracellular neurofibrillary tangles of filaments containing the hyperphosphorylated protein tau (3, 4). Accelerated deposition of Aβ deposits seems to be a key risk factor associated with AD, and although the mechanisms of the disease are still not fully understood, reducing the deposition of amyloid plaques seems to benefit patients.

Several radioligands for positron emission tomography (PET) have been developed (5-7) and tested in humans as in vivo diagnostic tools for imaging Aβ deposits (7). The first successful agent used in human studies was [^18^F]FDDNP (8), a malonitrile derivative found to bind to both neurofibrillary tangles and β-amyloid plaques. The second compound was [^11^C]PIB (9), also known as Pittsburgh Compound B or [^11^C]6-OH-BTA-1. [^11^C]PIB showed marked retention in areas of association cortex known to contain substantial amounts of Aβ deposits. The third PET radioligand tested in humans was [^11^C]4-N-methylamino-4´-hydroxystilbene, a stilbene derivative commonly named [^11^C]SB-13 that exhibited good binding affinities for Aβ aggregates in vitro, moderate lipophilicity, high initial brain uptake in the normal rat cortex, and a rapid washout (10).

Other imaging agents based on benzofuran derivatives labeled with radioactive iodine have shown very good binding affinities for Aβ aggregates and good brain penetration (11). Unfortunately, their level of nonspecific binding was found to be very high, making them unsuitable for in vivo plaque imaging. However, [^125^I]IMPY displayed a good initial brain uptake and rapid washout from normal mouse brain and postmortem AD brain sections (12).

A series of novel probe for β-amyloid plaques using derivatives of curcumin are currently under investigation in vitro and in small animals. Curcumin, a natural compound studied for its antioxidant and anticancer properties, has shown have favorable brain permeability and Aβ plaque binding properties by fluorescence staining in brain section of APPsw transgenic mice (13). Preliminary research studies have shown that [^18^F]Fluropropyl-substituted curcumin (1-[4-(3-[^18^F]fluoropropoxy)-3-methoxyphenyl]-5-hydroxy-7-(4-hydroxy-3-methoxyphenyl)-1,4,6-heptatrien-3-one) might be a suitable radioligand for Aβ plaque imaging using PET (14).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29Fluoropropyl-substituted%20curcumin%20AND%20synthesis)]

[^18^F]Fluropropyl-substituted curcumin can be synthesized using the method described by Ryu et al. (14). This method uses the coupling of a keto-enol compound with the corresponding vanillin derivative-boron complex in the presence of piperidine (which leads to better yields than by using n-butylamine). Briefly, [^18^F]Fluropropyl-substituted curcumin (1-[4-(3-[^18^F]fluoropropoxy)-3-methoxyphenyl]-5-hydroxy-7-(4-hydroxy-3-methoxyphenyl)-1,4,6-heptatrien-3-one) is prepared from [^18^F]4-(3-fluoropropoxy)-3-methoxybenzaldehyde, which is itself synthesized from reacting 4-(3-tosyloxypropoxy)-3-methoxybenzaldehyde together with n-Bu_4_N[^18^F]F. Further details can be found in the following reference (14).

The subsequent aldol condensation with acetylacetone-boron complex, followed by HPLC purification, gave the product in overall decay-corrected radiochemical yield of 16-25%, and with a radiochemical purity >98%. The total synthesis time for [^18^F]Fluropropyl-substituted curcumin was ~ 120 min. The effective specific activity measured at the end of synthesis was 37.6 GBq/µmol (1.6 Ci/µmol) (14) .

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29Fluoropropyl-substituted%20curcumin%20AND%20in%20vitro)]

In vitro binding assays were performed by Ryu et al. (14), as previously described in the literature (15, 16). Results showed that curcumin exhibited potent binding affinity for Aβ aggregates (K_i_ = 0.20 nM). Additionally, it was shown that the introduction of an iodine into its phenyl ring significantly decreased its binding affinity by 47-fold, whereas O-fluoropropylation of its hydroxyl group increased binding its binding affinity by 2.9-fold (leading to K_i_ = 0.07 nM). The partition coefficient (P) for [^18^F]Fluropropyl-substituted curcumin, measured using an octanol-water mixture, led to a value of log P = 1.84, predicting a favorable brain permeability.

Metabolic studies performed by Ryu et al. (14) using mouse brain and blood showed that [^18^F]Fluropropyl-substituted curcumin remained intact in the brain during the time of the study (60 min), whereas an unidentified polar metabolite appeared in blood samples within 2 min after injection of the radiotracer. [^18^F]Fluropropyl-substituted curcumin was found to be completely converted into the metabolite at 60 min post injection (Figure 2). This polar radioactive metabolite did not appear to cross the BBB, due to its high polarity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29Fluoropropyl-substituted%20curcumin%20AND%20%28mice%20OR%20rodentia%5BMeSH%5D%29)]

Ryu et al. (14) conducted ex vivo preliminary studies of [^18^F]fluropropyl-substituted curcumin in four normal male mice (25-30 g each) to assess its ability to cross the brain blood barrier (BBB). After injection of 1.85 MBq (0.05 mCi) by the tail vein, the animals were sacrificed and the radioactivity was counted on weighted organs, at different point in times. The reported value for the radiotracer initial uptake was ≈ 0.69% of the injected dose (ID)/g. At 2 min post injection, the measured uptake was 0.52% ID/g. A rapid washout from the brain was obtained in 30 min (with uptake values ≈ 0.11% ID/g at 30 and 60 min post injection).

Biodistribution studies showed a high and persistent level of radioactivity uptake in the liver and spleen, while the uptake in the lungs decreased with time. Reported uptake values (in %ID/g ± standard deviation) at 2, 30 and 60 min post injection were as follows: 38.99 ± 2.80, 41.06 ± 5.41 and 37.06 ± 6.24 for the liver, 16.32 ± 1.99, 42.94 ± 1.19, 36.05 ± 9.45 for the spleen, 30.91 ± 4.43, 7.23 ± 0.34, 10.55 ± 1.73 for the lung, 4.05 ± 0.40, 0.57 ± 0.08 and 0.64 ± 0.08% for the heart.

[^18^F]Fluropropyl-substituted curcumin did not appear to undergo metabolic defluorination from bone uptake, which values were found to remain constant over time (2.7-3.4%ID/g). The relatively low initial brain uptake might be explained by the rapid metabolism of [^18^F]Fluropropyl-substituted curcumin in the liver and in the intestinal wall, as observed with ‘native’ curcumin (17). Because piperine (a major component of black pepper and known inhibitor of hepatic and intestinal glucuronidation) was shown to dramatically increase the bioavailability of curcumin (17) by oral co-administartion, Ryu et al. (14) explored the effect of piperine on the uptake of [^18^F]Fluropropyl-substituted curcumin. Results showed that a co-injection of piperine with [^18^F]Fluropropyl-substituted curcumin in normal mice led to an increase of the initial brain uptake by ≈ 48% (0.77% ID/g with piperine vs. 0.52% ID/g without piperine, at 2 min post injection), whereas other organ uptakes were found similar to those without piperine. As noted by the authors, the effect of piperine was limited, possibly due to its poor solubility in 10% ethanol-saline used in the experiments (14).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29Fluoropropyl-substituted%20curcumin%20AND%20%28dog%20OR%20sheep%20OR%20pig%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29Fluoropropyl-substituted%20curcumin%20AND%20%28baboon%20OR%20%28primate%20NOT%20human%29%29)](14)

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29Fluoropropyl-substituted%20curcumin%20AND%20human)]

No publication is currently available.

## References

1 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci, . 11 Spec No: p. 213-328.
2 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
3 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
4 Brandt R., Leschik J. (2004). Functional interactions of tau and their relevance for Alzheimer's disease. Curr Alzheimer Res.
5 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
6 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
7 Wu C., Pike V.W., Wang Y. (2005). Amyloid imaging: from benchtop to bedside. Curr Top Dev Biol.
8 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
9 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
10 Ono M., Wilson A., Nobrega J., Westaway D., Verhoeff P., Zhuang Z.P., Kung M.P., Kung H.F. (2003). 11C-labeled stilbene derivatives as Abeta-aggregate-specific PET imaging agents for Alzheimer's disease. Nucl Med Biol.
11 Ono M., Kung M.P., Hou C., Kung H.F. (2002). Benzofuran derivatives as Abeta-aggregate-specific imaging agents for Alzheimer's disease. Nucl Med Biol.
12 Kung M.P., Hou C., Zhuang Z.P., Zhang B., Skovronsky D., Trojanowski J.Q., Lee V.M., Kung H.F. (2002). IMPY: an improved thioflavin-T derivative for in vivo labeling of beta-amyloid plaques. Brain Res.
13 Yang F., Lim G.P., Begum A.N., Ubeda O.J., Simmons M.R., Ambegaokar S.S., Chen P.P., Kayed R., Glabe C.G., Frautschy S.A., Cole G.M. (2005). Curcumin inhibits formation of amyloid beta oligomers and fibrils, binds plaques, and reduces amyloid in vivo. J Biol Chem.
14 Ryu E.K., Choe Y.S., Lee K.H., Choi Y., Kim B.T. (2006). Curcumin and dehydrozingerone derivatives: synthesis, radiolabeling, and evaluation for beta-amyloid plaque imaging. J Med Chem.
15 Zhuang Z.P., Kung M.P., Hou C., Skovronsky D.M., Gur T.L., Plossl K., Trojanowski J.Q., Lee V.M., Kung H.F. (2001). Radioiodinated styrylbenzenes and thioflavins as probes for amyloid aggregates. J Med Chem.
16 Klunk W.E., Wang Y., Huang G.F., Debnath M.L., Holt D.P., Mathis C.A. (2001). Uncharged thioflavin-T derivatives bind to amyloid-beta protein with high affinity and readily enter the brain. Life Sci.
17 Shoba G., Joy D., Joseph T., Majeed M., Rajendran R., Srinivas P.S. (1998). Influence of piperine on the pharmacokinetics of curcumin in animals and human volunteers. Planta Med.